# Annexin B12 Cys101,Cys260-N,N'-dimethyl-N-(iodoacetyl)-N'-(7-nitrobenz-2-oxa-1,3-diazol-4-yl)ethylenediamine

Chemical name: | Annexin B12 Cys101,Cys260-N,N'-dimethyl-N-(iodoacetyl)-N'-(7-nitrobenz-2-oxa-1,3-diazol-4-yl)ethylenediamine
Abbreviated name: | pSIVA_m_
Synonym: | AnxB12 Cys101,Cys260-IANBD
Agent Category: | Proteins
Target: | Phosphatidylserine
Target Category: | Lipids
Method of detection: | Optical imaging
Source of signal / contrast: | N,N'-dimethyl-N-(iodoacetyl)-N'-(7-nitrobenz-2-oxa-1,3-diazol-4-yl)ethylenediamine (IANBD)
Activation: | Yes
Studies: | - In vitro; - Rodents | No structure is available.

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed/?term=apoptosis+and+annexins+and+imaging)]

Apoptosis, or programmed cell death, presents specific biochemical changes at its different stages (1-4). By targeting changes such as exposed phosphatidylserine (PS), dysfunctional mitochondria, activated caspases, fragmented DNA, and disrupted membrane integrity, various apoptosis-detecting methods have been developed and provide diagnostic and prognostic value for human diseases, most notably for cancer, myocardial dysfunction, and neurodegenerative disorders (2-5). For several reasons, exposed PS has been used as a single and direct target for apoptosis detection (2, 6-10) although it is not specific for apoptosis. First, PS is normally limited to the inner leaflet of the plasma membrane bilayer, whereas it is externalized to the outer leaflet of the membrane in the presence of calcium ions during apoptosis. Second, cell surface exposure of PS has been considered to be an indicator of early apoptotic processes in the absence of necrosis. Therefore, monitoring PS exposure provides a way to observe the initiation of the apoptotic pathway before other changes are present. Third, PS exposure provides extracellular binding targets that can be detected without the need to penetrate the cells.

Annexins are cellular proteins that are widely used to design PS-targeted, apoptosis-detecting probes (1, 7, 9). Annexins are characterized by their calcium-dependent ability to bind to negatively charged PS. All annexins are composed of two distinct regions: a C-terminal core and an amino N-terminal “head” region. The annexin core is highly conserved across the annexin family, and the N-terminus varies greatly. Radiolabeled annexin derivatives have already been used for clinical imaging in many diseases (2, 8, 10). However, annexin-based probes suffer from several drawbacks, such as slow delivery to the site of interest, slow clearance from tissue leading to high effective doses, and low specificity. Annexin-based probes do not appear to distinguish apoptosis from necrosis. Furthermore, PS externalization is associated with inflammation and platelet activation, causing further challenges with annexin-based probe specificity.

To address these problems, Kim et al. developed a class of polarity-sensitive annexin-based probes (pSIVAs) with built-in "on" (membrane-bound) and "off" (in solution) fluorescent states (1). The probes were generated by placing polarity-sensitive thiol-reactive fluorophores in the loop regions of annexin B12 (anxB12, also known as annexin XII) or annexin A5 (anx5, also known as annexin V), taking advantage of loop region mediation of Ca^2+^-dependent membrane interactions, transitioning from a polar (aqueous solution) to a nonpolar (lipid membrane) environment upon membrane binding. Two thiol-reactive fluorophores, N,N'-dimethyl-N-(iodoacetyl)-N'-(7-nitrobenz-2-oxa-1,3-diazol-4-yl)ethylenediamine (IANBD) and 6-bromoacetyl-2-dimethylaminonaphthalene (BADAN), were tested, and the resulting probes were evaluated for apoptosis detection. The results showed that probe binding with PS on the apoptotic cells resulted in a measurable increase in fluorescence emission intensity. pSIVA_m_ (also known as anxB12 Cys101,Cys260-IANBD) is one of the promising probes for apoptosis detection (1).

### Related Resource Links:

- Chapters of annexin-based probes in MICAD (http://www.ncbi.nlm.nih.gov/sites/entrez?db=Books&cmd=Search&term=annexin+AND+micad%5bbook%5d&doptcmdl=TOCView&log%24=booksrch&bname=micad)
- Clinical trials of annexin-based probes in ClinicalTrials.gov (http://clinicaltrials.gov/ct2/results?term=annexin+and+imaging)
- Gene information for human annexins (http://www.ncbi.nlm.nih.gov/gene/?term=annexin+human)
- Annexin information in OMIM (http://www.ncbi.nlm.nih.gov/omim/?term=annexins)
- Annexin-related substances in PubChem (http://www.ncbi.nlm.nih.gov/pcsubstance/?term=annexin)
- Apoptosis-related bioassay in PubChem (http://www.ncbi.nlm.nih.gov/pcassay/?term=apoptosis)

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed/19966809)]

Kim et al. screened for polarity-sensitive molecules that emit increased fluorescence intensity in nonpolar environments, and the investigators selected two thiol-reactive fluorophores, IANBD and BADAN, as reporters (detailed data not shown) (1). AnxB12 and anxA5 proteins with cysteine mutations were then generated in cysteine-less variants of anxA5 (C316A) and anxB12 (C113A, C302A) plasmids with site-directed mutagenesis. The mutant protein products were expressed, purified, and reacted with a ten-fold molar excess of IANBD or BADAN at the introduced cysteine sites. The generated probes included IANBD- or BADAN-labeled anxA5 Cys262, anxB12 Cys4, anxB12 Cys101, and anxB12 Cys101,Cys260. The probe pSIVA_m_ was referred to the anxB12 labeled at both residue positions 101 and 260 with IANBD (anxB12 Cys101,Cys260-IANBD). Kim et al. also generated two negative control probes (anxB12 Cys4-IANBD and anxB12 Cys4-BADAN) by labeling residue 4 in the N-terminal tail of anxB12, which were expected to stay fully exposed to the aqueous environment in both the solution and membrane-bound states (1). The purity, labeling efficiency, and yield of the probes were not described in detail.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed/19966809)]

Kim et al. evaluated the differences in the fluorescence emission of the probes between the solution and membrane-bound states with in vitro binding assay (1). The fluorescence intensity was negligible for all probes free in solution and for the negative control molecules in both in-solution and membrane-bound states. Considerable increases in fluorescence intensity were measured for all probes in their membrane-bound states, suggesting binding to membrane PS. The membrane-bound pSIVA_m_ exhibited fluorescence ~45-fold greater than that found in the in-solution state, and the membrane-bound pSIVA_m_ was brighter than other membrane-bound probes. Slightly lower fluorescence intensities were detected for BADAN-labeled probes than for corresponding IANBD-labeled probes. There was no detectable decrease in membrane binding or loss of specificity to PS for all probes. These results indicate that attachment of polarity-sensitive IANBD and BADAN to cysteine residues in the membrane-binding loops provides an effective way to generate annexin derivatives with built-in "on" and "off" fluorescent states.

To test the application of pSIVA_m_ to image live cells undergoing apoptosis, Kim et al. added pSIVA_m_ directly to cultured COS-7 cells that had been induced to undergo apoptosis by etoposide (1). As expected, the investigators observed bright pSIVA_m_ staining of the COS-7 cells at the early stages of apoptosis and a gradual increase in staining concurrent with progression into late-stage cell death. In comparison, no staining was observed for cells grown under normal conditions, suggesting that pSIVA_m_ binding and fluorescence emission were specific to apoptotic cells. The background fluorescence from the in-solution state was undetectable. pSIVA_m_ did not influence the cell growth (data not shown).

Kim et al. next determined whether pSIVA_m_ could be used to study axonal degeneration using purified primary dorsal root ganglion (DRG) sensory neurons (1). DRG neurons have a single axon without dendrites, and under various conditions axonal degeneration and death occur at different times and independently from each other. In addition, DRG neurons are dependent on trophic factor support for survival. The investigators observed pSIVA_m_ staining in both axons and cell bodies of nerve growth factor (NGF)-deprived neurons, whereas pSIVA_m_ staining was largely absent in neurons grown in the presence of NGF. The fluorescence intensity increased gradually in the NGF-deprived neurons, corresponding to both a gradual increase in the amount of PS exposure in an individual neuron and the number of degenerating neurons present over longer periods of NGF deprivation. pSIVA_m_ binding occurred in a specific spatiotemporal order, which indicates that PS exposure occurred successively, originating from a particular location in the axon and progressing toward the cell body. The dynamic, sequential, punctate staining pattern observed in the axons was characteristic of binding to the PS exposed on the outer leaflet of the plasma membrane rather than binding to the PS from the intracellular side, where PS is more abundant and uniformly distributed.

Axonal degeneration is a highly regulated dynamic process that does not necessarily result in cell death. Understanding the temporal dynamics of whether and when rescue is possible in degenerating neurons will provide an indication of the severity of the cellular response and the time window in which neuronal survival mechanisms can still be effective (1-3). Therefore, Kim et al. first initiated degeneration in DRG neurons by NGF deprivation and then added back NGF once they detected PS exposure on the axons (at 7, 10, and 15 h after initial NGF removal) (1). Complete cell death was blocked with re-administration of NGF in some cells but not all. Concurrent with neuronal survival after replacing NGF, the investigators observed a decrease in pSIVA_m_ staining fluorescence, indicating that binding decreased as PS was restored to the inner leaflet of the plasma membrane. For neurons that were deprived of NGF for 15 h before replenishing NGF, maximum fluorescence intensity was reached at 20–24 h, followed by a decrease to the end of the 40-h time course. On the other hand, when the neurons were continuously deprived of NGF, pSIVA_m_ fluorescence increased and was maintained to the end of the experiment. Therefore, Kim et al. observed rescue from degeneration in neurons with pSIVA_m_-stained axons but not in neurons with pSIVA_m_-stained cell bodies, which was indicative of later stages of cell death. Some axons retained pSIVA_m_ staining after the re-administration of NGF, indicating that rescue was not possible in intermediate stages. These results indicate that there is a critical period after the initiation of apoptotic mechanisms in which rescue is still possible (after PS exposure in the axon but before PS exposure in the cell body) (1).

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed/19966809)]

To test the utility of pSIVAs for in vivo applications, Kim et al. administered pSIVA_m_ by intramuscular injection along the rat sciatic nerve 3 days after nerve transection and then imaged the degenerating neurons (1). pSIVA_m_ exclusively stained axons in the sciatic nerve distal to the site of injury, whereas staining in the contralateral control (uninjured) sciatic nerve was undetectable. A dynamic punctate staining pattern in the sciatic nerve axons was observed, which was similar to the findings in degenerating axons of DRG neurons in vitro.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%22%20SUBSTANCENAME%22%5BSubstance%20Name%5D%20AND%20%28dog%20OR%20rabbit%20OR%20pig%20OR%20sheep%29)]

No references are currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%22SUBSTANCENAME%22%5BSubstance%20Name%5D%20AND%20%28primate%20NOT%20human%29)]

No references are currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%22SUBSTANCENAME%22%5BSubstance%20Name%5D%20AND%20human)]

No references are currently available.

## References

1 Kim Y.E., Chen J., Chan J.R., Langen R. (2010). Engineering a polarity-sensitive biosensor for time-lapse imaging of apoptotic processes and degeneration. Nat Methods.
2 Smith G., Nguyen Q.D., Aboagye E.O. (2009). Translational imaging of apoptosis. Anticancer Agents Med Chem.
3 Tait J.F. (2008). Imaging of apoptosis. J Nucl Med.
4 Blankenberg F.G. (2008). In vivo detection of apoptosis. J Nucl Med.
5 De Saint-Hubert M., Prinsen K., Mortelmans L., Verbruggen A., Mottaghy F.M. (2009). Molecular imaging of cell death. Methods.
6 Belhocine T.Z., Blankenberg F.G. (2006). The imaging of apoptosis with the radiolabelled annexin A5: a new tool in translational research. Curr Clin Pharmacol.
7 van Genderen H.O., Kenis H., Hofstra L., Narula J., Reutelingsperger C.P. (2008). Extracellular annexin A5: functions of phosphatidylserine-binding and two-dimensional crystallization. Biochim Biophys Acta.
8 Laufer E.M., Reutelingsperger C.P., Narula J., Hofstra L. (2008). Annexin A5: an imaging biomarker of cardiovascular risk. Basic Res Cardiol.
9 Monastyrskaya K., Babiychuk E.B., Draeger A. (2009). The annexins: spatial and temporal coordination of signaling events during cellular stress. Cell Mol Life Sci.
10 Chun H.J., Narula J., Hofstra L., Wu J.C. (2008). Intracellular and extracellular targets of molecular imaging in the myocardium. Nat Clin Pract Cardiovasc Med.